# PEGylated paramagnetic lipid-coated silica nanoparticles with a fluorescent quantum dot core

Chemical name: | PEGylated paramagnetic lipid-coated silica nanoparticles with a fluorescent quantum dot core
Abbreviated name: | Q-SiPaLCs
Synonym:
Agent Category: | Nanoparticles
Target: | Non-targeted
Target Category:
Method of detection: | Multimodal imaging (magnetic resonance imaging and optical imaging)
Source of signal / contrast: | Gd and quantum dot (QD)
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=multimodal%20imaging%20agent)]

The PEGylated paramagnetic lipid-coated silica nanoparticle with a fluorescent quantum dot (QD) core, abbreviated as Q-SiPaLCs, is a bimodal imaging agent that has been developed by Koole et al. and van Schooneveld et al. for combined magnetic resonance imaging (MRI) and optical imaging (1-3).

The idea of using multiple modalities in a single imaging session comes from the fact that imaging modalities with high sensitivity have relatively poor resolution, while those with high resolution have relatively poor sensitivity (4, 5). Integration of multiple modalities in imaging would combine the advantages of each modality and allow better characterization of diseases and disease processes (6). Development of hybrid imaging technology has also triggered great effort in the development of multimodal imaging agents to boost the benefits of hybrid instrument technology (7, 8).

In principle, the synthesis of multimodal agents is similar to that of single-mode agents (8). A large molecule is usually necessary for efficient labeling and delivery of multiple reporters. Intensively investigated large molecules include liposomes, dendrimers, polymers, and endogenous nanoparticles (8, 9). In the case of liposomes, reporters are either encapsulated in the aqueous interior space or incorporated into the lipid bilayer (1, 2). The latter approach usually results in an improved ionic relaxivity of the MRI metals. In the development of multimodal agents, questions arise from the multistep conjugations that often lead to a low chemical yield. The presence of different molecules on the same nanoparticle surface may interfere with the targeting capabilities and the subsequent intracellular uptake of the agents. The optimization of multimodal imaging agents is more challenging in terms of immunogenicity, toxicity, specificity, interference with biological processes, and accumulation in target organs (7, 8).

Koole et al. and van Schooneveld et al. synthesized a series of multimodal imaging agents by coating silica particles with a dense monolayer of PEGylated paramagnetic lipids without the use of coupling agents (1-3). The presence of a dense lipid layer around the inorganic particle core renders these particles stable in aqueous dispersion and bioapplicable. The lipid coating also allows for conjugation of target-specific molecules at the surface. These agents include Q-SiPaLCs, RGD-conjugated Q-SiPaLCs, and Au-SiFluPaLCs. Of these agents, Q-SiPaLCs were synthesized as a bimodal contrast agent for combined MRI and optical imaging (2, 3). This bimodal agent is composed of a silica-coated QD core with a PEGylated paramagnetic lipid coating (1). The QD core enables its detection with optical imaging, while the paramagnetic lipids generate the MRI signal. This agent has been characterized in vitro and in mice (2, 3). This chapter summarizes the data obtained with Q-SiPaLCs. Another chapter in MICAD summarizes the data obtained with Au-SiFluPaLCs (http://www.ncbi.nlm.nih.gov/books/NBK5330/).

### Related Resource Links:

Multimodal imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=multimodality+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=19035793)]

Koole et al. described the synthesis of Q-SiPaLCs and characterized the particles in detail (2). CdSe QDs (3.4 nm in diameter) were synthesized via the conventional organometallic synthesis route. The QDs were coated with seven monolayers of inorganic shells (2 × CdSe, 3 × Cd_0.5_Zn_0.5_Se, 2 × ZnSe). The resulting core-shell-shell QDs (CSS-QDs) increased to 7.7 ± 0.9 nm in diameter with a quantum yield (QY) of 60% and were photostable in air for months. The CSS-QDs were incorporated in silica spheres by a reverse microemulsion method. The silica-coated QDs were subsequently capped with hydrophobic octadecanol (ODOH), at which point the ODOH-coated silica nanoparticles were dispersed in chloroform/methanol and further coated with PEGylated paramagnetic lipids. The PEGylated paramagnetic lipids were prepared with 1,2-distearoyl-sn-glycero-3-phosphoethanolamine-N-[methoxy(poly(ethylene glycol))-2000] (PEG-DSPE), 1,2-distearoyl-sn-glycero-3-phosphoethanolamine-N-[maleimide-(poly(ethylene glycol))2000] (Mal-PEG-DSPE), and gadolinium diethylenetriamine pentaacetic acid-di(stearylamide) (Gd-DTPA-DSA) in a molar ratio of 0.4/0.1/0.5.

Negative stain transmission electron microscopy (TEM) revealed a hydrophobic layer of 3.9 ± 0.5 nm around individual particles, confirming the presence of ODOH coating around the silica (~2 nm) and the stearyl chains of the lipids (~2 nm) around the particles (2). The hydrodynamic diameter was estimated to be 50 nm for ODOH-coated particles, which increased to 58 nm after lipid coating, as determined with dynamic light scattering. The absorption spectrum of the nanoparticles displayed multiple absorption features as a result of discrete excitonic transitions in the CSS-QDs, which can be observed due to the high quality and monodispersity of QDs. The initial QY of the CSS-QDs decreased from 65% to 25% after the silica coating, however the QY was difficult to be measured because of the scattering of the silica particles in ethanol. The QY increased to 35% after capping with ODOH, which could be accurately determined because of the scattering-free dispersion of the hydrophobic particles in chloroform. The silica coating and further coating steps did not change the shape of absorption or emission spectra of the QDs. The emission maximum of the CSS-QDs was ~630 nm.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=19035793)]

The longitudinal relaxivity r_1_ of the Q-SiPaLCs was calculated to be 14.4 mM^-1^s^-1^, which is three to four times higher than that of the free Gd-chelate molecules (2). This difference is ascribed to the lower tumbling rate of the Gd-lipids in the micelle compared to free Gd-DTPA-DSA. The r_2_/r_1_ ratio was 1.6, indicating that Q-SiPaLCs can be used as an effective T1 agent. The r_2_/r_1_ ratio is often used to determine whether a contrast agent is more suitable for T1-weighted or for T2-weighted MRI.

Inductively coupled plasma mass spectrometry (ICP-MS) showed that the number of Gd-lipids was 2,500 per silica particle, and it was estimated that half of the lipids carried Gd-DTPA-DSA (2).

Cell viability was determined with murine J744A.1 macrophages after incubation with different concentrations of Q-SiPaLCs or bare silica particles (3). After incubation with Q-SiPaLCs for 1 d and 3 d, the number of surviving cells was found to be considerably higher than the number of surviving cells after incubation with bare silica particles. The investigators observed no significant difference in cell survival between Q-SiPaLCs and bare silica particles after incubation for 2 h.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%22van%20Schooneveld%20MM%22%5bAuthor%5d)]

van Schooneveld et al. determined the half-life of Q-SiPaLCs with C57bl6 mice (n = 2/time point) (3). The cadmium (Cd) half-lives in plasma were 14 ± 2 min and 162 ± 34 min for the bare and lipid-coated silica nanoparticles, respectively, as determined with ICP-MS. These values closely resembled the half-lives as determined with fluorescence imaging, which were 18 ± 3 min for bare nanoparticles and 165 ± 28 min for lipid-coated nanoparticles. The molar Gd/Cd ratio in blood had a constant average value of 2.95 ± 0.34 at all time points after injection of the Q-SiPaLCs, which was identical to that of the Q-SiPaLCs before injection. These results indicated that the paramagnetic lipids did not dissociate from the nanoparticles in the blood.

Dynamic MRI of the aorta was performed at 9.4 T (n = 3 mice) and showed clear enhancement of the vasculature for at least 2 h after intravenous administration of the Q-SiPaLCs (45 μmol Gd/kg) compared to the prescan (3).

Optical imaging was performed for liver, spleen, kidney, and heart from mice euthanized at 1, 4, and 24 h after injection of the nanoparticles (n = 2 mice/time point) (3). The fluorescence signal in the liver of mice injected with Q-SiPaLCs increased gradually with time, while a negligible fluorescence signal was obtained from the spleen, heart, and kidney. The fluorescence intensity in the liver did not reach its maximum value until 4 h after injection. In the case of the bare silica particles, the fluorescence signal from the liver increased greatly, whereas the signals from the spleen, heart, and kidney were negligible. Contrary to the Q-SiPaLCs, maximum fluorescence signal in the liver was observed as early as 1 h after injection.

Organ distribution of the particles was determined with ICP-MS by determining the Cd content in organs (n = 1 mouse/time point and particle) (3). Fourteen nmol/kg particles of either lipid-coated or bare silica nanoparticles were administered intravenously into C57bl6 mice, which resulted in calculated 1.1 μmol Gd per mice (or 45 μmol/kg). Cd determinations allowed for comparison between the Q-SiPaLCs and bare silica particles because both types of particles contain equal amounts of this element. Similar to the optical imaging results, ICP-MS showed that the Q-SiPaLCs accumulated gradually in the liver, whereas negligible amounts of Cd were found in the kidney, lung, and heart. In contrast to the optical imaging results, a gradual uptake of the Q-SiPaLCs was also observed in the spleen. This discrepancy was also observed for the bare silica particles and was attributed to the high absorbance of the QD emission by the spleen. Bare silica particles accumulated within 1 h in the liver, lung, and spleen to a greater extent than that observed with Q-SiPaLCs, leading to breathing problems and liver necrosis. Three of 11 mice died after bare silica particles were administered, whereas no acute adverse effects were observed after the administration of Q-SiPaLCs.

The distribution of Q-SiPaLCs at the cellular level was investigated with confocal scanning laser microscopy and TEM (3). Mice were euthanized 24 h after particle injection, and organ sections were taken from the liver, spleen, kidney, lung, and heart. The Q-SiPaLCs and bare silica particles were observed in the liver and spleen, and bare silica particles were also observed in the lung. The macrophage stain revealed a high degree of colocalization between both types of particles and macrophages. The Q-SiPaLCs were localized in the lysosomal parts of macrophages and remained well dispersed in the organs; bare silica particles aggregated to a much larger extent, and the aggregates were mostly found in or adjacent to blood vessels. In the lung, aggregates were also found to block the capillaries.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 van Schooneveld M.M., et al. (2010). A fluorescent, paramagnetic and PEGylated gold/silica nanoparticle for MRI, CT and fluorescence imaging. Contrast Media Mol Imaging.
2 Koole R., et al. (2008). Paramagnetic lipid-coated silica nanoparticles with a fluorescent quantum dot core: a new contrast agent platform for multimodality imaging. Bioconjug Chem.
3 van Schooneveld M.M., et al. (2008). Improved biocompatibility and pharmacokinetics of silica nanoparticles by means of a lipid coating: a multimodality investigation. Nano Lett.
4 Cherry S.R. (2006). Multimodality in vivo imaging systems: twice the power or double the trouble?. Annu Rev Biomed Eng.
5 Cherry S.R. (2009). Multimodality imaging: beyond PET/CT and SPECT/CT. Semin Nucl Med.
6 Jennings L.E., Long N.J. (2009). 'Two is better than one'--probes for dual-modality molecular imaging. Chem Commun (Camb).
7 Lee S., Chen X. (2009). Dual-modality probes for in vivo molecular imaging. Mol Imaging.
8 Louie A. (2010). Multimodality imaging probes: design and challenges. Chem Rev.
9 Alric C., et al. (2008). Gadolinium chelate coated gold nanoparticles as contrast agents for both X-ray computed tomography and magnetic resonance imaging. J Am Chem Soc.